# [^11^C]5-Hydroxy-2-(4-methyaminophenyl)benzofuran

Chemical name: | [^11^C]5-Hydroxy-2-(4-methyaminophenyl)benzofuran
Abbreviated name:
Synonym:
Agent Category: | Compound
Target: | Aggregates of ß-amyloid (Aß) peptides
Target Category: | Acceptor binding
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=5-hydroxy-2-%284-methyaminophenyl%29benzofuran)]

Alzheimer’s disease (AD) is a major neurodegenerative disease associated with cognitive impairment and an irreversible decline of mental functions (1, 2). It is characterized by presence in the brain of senile plaques of β-amyloid (Aβ) peptides with intracellular neurofibrillary tangles of filaments that contain the hyperphosphorylated protein tau (3, 4). Accelerated deposition of Aβ deposits seems to be a key risk factor associated with AD, and although the mechanisms of the disease are still not fully understood, reducing the deposition of amyloid plaques seems to benefit patients.

Several radioligands for positron emission tomography (PET) have been developed (5-7) and tested in humans as in vivo diagnostic tools for imaging and measuring the formation and Aβ deposits (5-7) The first successful agent used in human studies was [^18^F]FDDNP (8), a malonitrile derivative found to bind to both neurofibrillary tangles and Aβ plaques. The second successful attempt was made with [^11^C]PIB (9), also known as Pittsburgh Compound B or [^11^C]6-OH-BTA-1. [^11^C]PIB showed marked retention in areas of the association cortex known to contain substantial amounts of Aβ deposits. The third PET radioligand tested in humans was [^11^C]4-N-methylamino-4´-hydroxystilbene, a stilbene derivative commonly named [^11^C]SB-13.

A series of benzofuran derivatives have recently been synthesized and are being evaluated as Aβ probes with PET. Probes that use radioactive iodine have shown very good binding affinities for Aβ aggregates and good brain penetration (10). Unfortunately, their level of nonspecific binding was found to be very high, which makes them unsuitable for in vivo plaque imaging. Other imaging agents that use benzofuran derivatives labeled with ^11^C are currently being evaluated. One of them, [^11^C]5-hydroxy-2-(4-methyaminophenyl)benzofuran , is currently being tested in small animals.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=5-hydroxy-2-%284-methyaminophenyl%29benzofuran%20AND%20synthesis)]

An experimental procedure for synthesizing 5-hydroxy-2-(4-methyaminophenyl)benzofuran was reported by Ono et al. (11) in 2006. The main step of the procedure involved the formation of the benzofuran backbone, 5-methoxy-2-(4-nitrophenyl)benzofuran, by an intramolecular Wittig reaction between triphenylphosphonium salt and 4-nitrobenzoyl chloride at a 33% yield. The Wittig reagent used in the procedure was prepared from 2-methoxy-5-hydroxybenzyl alcohol and triphenylphosphine hydrobromide at 84% yield.

5-Methoxy-2-(4-aminophenyl)benzofuran was converted to the monomethylamino derivative 5-methoxy-2-(4-methylaminophenyl)benzofuran by reducing the nitro group to an amino group with SnCl_2_ and subsequently monomethylating the amino group. 5-Methoxy-2-(4-aminophenyl)benzofuran was also converted to the dimethylamino derivative 5-methoxy-2-(4-dimethylaminophenyl)benzofuran at a 39% yield by a previously described method that uses paraformaldehyde, sodium cyanoborohydride, and acetic acid (11). The removal of the O-methyl groups (using BBr_3_) led to the formation of 5-hydroxy-2-(4-aminophenyl)benzofuran, the precursor used in the radiolabelling procedure of -hydroxy-2-(4-methyaminophenyl)benzofuran with ^11^C-labeled methyl triflate.

The final product, [^11^C]5-hydroxy-2-(4-methyaminophenyl)benzofuran, was obtained at a 21% yield (decay-corrected to end of bombardment) and with a radiochemical purity >99% . Its specific activity at the end of synthesis was ≈37 GBq/µmol (1 Ci/µmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=5-hydroxy-2-%284-methyaminophenyl%29benzofuran%20AND%20in%20vitro)]

In vitro binding assays using AD brain gray matter homogenates showed that [^11^C]5-hydroxy-2-(4-methyaminophenyl)benzofuran had a high binding affinity to amyloid plaques with an inhibition constant of 0.7 ± 0.2 nM. Measurements of the partition coefficient (P) in 1-octanol/phosphate buffer (pH 7.4) led to a log P value of 2.36 (11), which is considered within the optimal lipophilicity range for crossing the blood-brain barrier.

In vitro fluorescent labeling of AD sections was performed by Ono et al. (11) to investigate the neuropathological staining of senile plaques by 5-hydroxy-2-(4-methyaminophenyl)benzofuran. Results showed staining of neuritic plaques and cerebrovascular amyloids. In addition, [^11^C]5-hydroxy-2-(4-methyaminophenyl)benzofuran also displayed high binding affinity for neurofibrillary tangles in the AD sections. It was shown in a previous study that a marked increase in the amount of neurofibrillary tangles in the hippocampus and entorhinal cortex occurred in the preclinical AD stage (12).

Overall, the results from neuropathological staining of human AD obtained for sections showed that 5-hydroxy-2-(4-methyaminophenyl)benzofuran could bind to amyloid plaques and neurofibrillary tangles with almost the same pattern of [^18^F]FDDNP or X-34 (13).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=5-hydroxy-2-%284-methyaminophenyl%29benzofuran%20AND%20rodentia%5BMeSH%5D)]

Ono et al. (11) performed biodistribution studies of [^11^C]5-hydroxy-2-(4-methyaminophenyl)benzofuran in four 6-week-old male ddY mice (i.e., a superior strain of mice widely used in pharmacological, toxicological, and drug efficacy studies) by intravenously injecting the animals with 3.7 MBq (0.1 mCi) of the radiotracer in saline solution. The experimental protocol involved sacrificing the animals at various points in time and counting the radioactivity of excised and weighed organs.

Results showed that [^11^C]5-hydroxy-2-(4-methyaminophenyl)benzofuran exhibited excellent brain uptake (4.8% of the injected dose (ID)/g of the brain at 2 min) and rapid washout (>90% of the radioactivity from the brain in 30 min or less, with values of 0.4 and 0.2% ID/g of the brain at 30 and 60 min, respectively). The precise mechanisms responsible for the rapid clearance of [^11^C]5-hydroxy-2-(4-methyaminophenyl)benzofuran from the normal brain are still unknown.

Ex vivo plaque labeling of amyloid plaques in a living mouse brain was performed by Ono et al. (11) by intravenously injecting 22-month-old female Tg2576 mice (i.e., AD mouse strain specifically engineered to overproduce the amyloid plaques in the brain) with 200 µl of a saline solution of ascorbic acid (1 mg/ml) and 7.4–9.3 MBq (0.2–0.25 mCi) of [^11^C]5-hydroxy-2-(4-methyaminophenyl)benzofuran. After sacrificing the animals, brain sections were cut and exposed to a phosphor imaging plate.

Autoradiographic images of brain sections at 30 min after injection of [^11^C]5-hydroxy-2-(4-methyaminophenyl)benzofuran showed high radioactivity accumulation in the cerebral cortex and hippocampus. In contrast, wild-type mouse brain displayed no remarkable accumulation of the radiotracer in the brain. In those studies, Ono et al. (11) showed that the most intense areas of staining in the brain sections of Tg2576 mice injected with [^11^C]5-hydroxy-2-(4-methyaminophenyl)benzofuran corresponded with those of in vitro thioflavin-S staining in the same brain sections.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=5-hydroxy-2-%284-methyaminophenyl%29benzofuran%20AND%20%28dog%20OR%20pig%20OR%20sheep%20OR%20cat%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=5-hydroxy-2-%284-methyaminophenyl%29benzofuran%20AND%20%28baboon%20OR%20%28primate%20NOT%20human%29%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=5-hydroxy-2-%284-methyaminophenyl%29benzofuran%20AND%20humans)]

No publication is currently available.

## References

1 Heininger K. (2000). . A unifying hypothesis of Alzheimer's disease. IV. Causation and sequence of events. Rev Neurosci, 11 Spec No: p. 213-328.
2 Forstl H, Kurz A. (1999). Clinical features of Alzheimer's disease. Eur Arch Psychiatry Clin Neurosci.
3 Hardy J. (2003). The relationship between amyloid and tau. J Mol Neurosci.
4 Brandt R, Leschik J. (2004). Functional interactions of tau and their relevance for Alzheimer's disease. Curr Alzheimer Res.
5 Nordberg A. (2004). PET imaging of amyloid in Alzheimer's disease. Lancet Neurol.
6 Bacskai BJ, Hickey GA, Skoch J, Kajdasz ST, Wang Y, Huang GF, Mathis CA, Klunk WE, Hyman BT. (2003). Four-dimensional multiphoton imaging of brain entry, amyloid binding, and clearance of an amyloid-beta ligand in transgenic mice. Proc Natl Acad Sci U S A.
7 Wu C, Pike VW, Wang Y. (2005). Amyloid imaging: from benchtop to bedside. Curr Top Dev Biol.
8 Shoghi-Jadid K, Small GW, Agdeppa ED, Kepe V, Ercoli LM, Siddarth P, Read S, Satyamurthy N, Petric A, Huang SC, Barrio JR. (2002). Localization of neurofibrillary tangles and beta-amyloid plaques in the brains of living patients with Alzheimer disease. Am J Geriatr Psychiatry.
9 Klunk WE, Engler H, Nordberg A, Wang Y, Blomqvist G, Holt DP, Bergstrom M, Savitcheva I, Huang GF, Estrada S, Ausen B, Debnath ML, Barletta J, Price JC, Sandell J, Lopresti BJ, Wall A, Koivisto P, Antoni G, Mathis CA, Langstrom B. (2004). Imaging brain amyloid in Alzheimer's disease with Pittsburgh Compound-B. Ann Neurol.
10 Ono M, Kung MP, Hou C, Kung HF. (2002). Benzofuran derivatives as Abeta-aggregate-specific imaging agents for Alzheimer's disease. Nucl Med Biol.
11 Ono M, Kawashima H, Nonaka A, Kawai T, Haratake M, Mori H, Kung MP, Kung HF, Saji H, Nakayama M. (2006). Novel benzofuran derivatives for PET imaging of beta-amyloid plaques in Alzheimer's disease brains. J Med Chem.
12 Price JL, Morris JC. (1999). Tangles and plaques in nondemented aging and "preclinical" Alzheimer's disease. Ann Neurol.
13 Styren SD, Hamilton RL, Styren GC, Klunk WE. (2000). X-34, a fluorescent derivative of Congo red: a novel histochemical stain for Alzheimer's disease pathology. J Histochem Cytochem.